# [^11^C]Choline

Chemical name: | [^11^C]Choline
Abbreviated name: | [^11^C]CH
Synonym: | [^11^C]Trimethylethanolamine; [^11^C]trimethyl-2-hydroxyethylammonium
Agent category: | Compound
Target: | Choline kinase
Target category: | Enzyme
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Choline%5BAll%20Fields%5D)]

Choline is an important component of phospholipids in the cell membranes. Tissues with increased metabolism will lead to an increased uptake of choline. Choline is phosphorylated by choline kinases (CHK) to phosphorylcholine within cells, and, after several biosynthetic processes, finally is integrated into phospholipids (1). Because tumor cells have a high metabolic rate, choline uptake is high in order to keep up with the demands with the synthesis of phospholipids in their cellular membranes (2). Positron emission tomography (PET) with [^11^C]Choline has been reported to be useful for the detection and differential diagnosis of brain tumors, prostate cancer, lung cancer, and esophageal cancer (3, 4), whereas [^18^F]2-fluoro-2-deoxyglucose (FDG) lacks of specificity or sensitivity (3).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Choline+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Choline kinase (http://www.ncbi.nlm.nih.gov/gene/1119)).
- Articles in OMIM (Choline kinase (http://www.ncbi.nlm.nih.gov/omim/612395))
- Clinical trials ([^11^C]Choline (http://www.clinicaltrials.gov/ct2/results?term=11C+Choline))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Choline%5BAll%20Fields%5D%20AND%20%28%22chemical%20synthesis%22%5BSubheading%5D%20OR%20chemical%20synthesis%5BText%20Word%5D%29)]

[^11^C]Methylcholine was produced by reacting [^11^C]methyliodide with 2-dimethylaminoethanol. Purified [^11^C]choline was produced with a measured specific activity of 11.1 GBq/μmol (>300 mCi/μmol) and a radiochemical purity >98% at 35 min after bombardment. The radiochemical yield for the synthesis and purification was approximately 22% (5). A new method of [^11^C]choline synthesis was achieved by the reaction of [^11^C]methyl iodide with dimethylaminoethanol at 120 ºC for 5 min. Purification was performed by evaporation of the reactants, followed by passage of the aqueous solution of the product through a cation-exchange resin cartridge. The total time required for obtaining the finished chemical was 25 min. Radiochemical yield was > 98% with radiochemical purity of > 98%. Chemical purity was > 90% (6). An automated synthesis of [^11^C]choline with a radiochemical yield of about 42% was reported (7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Choline%5BAll%20Fields%5D%20AND%20in%20vitro)]

Because of the short half-life (20 min) of ^11^C, [^14^C]choline and [^3^H]choline were often used in in vitro studies. Both [^14^C] and [^3^H]choline were rapidly incorporated into phospholipids into PC-3 human prostate cancer cell line (1) and human astrocytoma cell line (8)

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Choline%5BAll%20Fields%5D%20AND%20rodentia)]

A biodistribution of [^11^C]choline was determined at 45 min post intravenous injection in nude mice transplanted with MCF-7 human breast cancer cell line or MDA-MB-435 human breast carcinoma. The results showed that the uptake of [^11^C]choline in these tumors was high, 2.0% dose/g in MCF-7 implanted mice and 1.8% dose/g in MDA-MB-435 implanted mice. The tumor/muscle ratios are moderate and the tumor/blood ratios are high. The major organs of [^11^C]Choline uptake were the kidneys, liver, small intestine, heart, and spleen. The micro-PET imaging of [^11^C]choline in both nude mice showed a clear uptake of [^11^C]choline in the transplanted breast tumors (9).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Choline%5BAll%20Fields%5D%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

[^11^C]Choline PET was studied in normal rabbits. [^11^C]Choline was taken up from blood by various tissues very rapidly, and the radioactivity remaining in blood became almost negligible 5 min after intravenous injection. The highest uptake was in the liver, followed by the kidneys and spleen at the end of this 36 min experiment (6)

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Choline%5BAll%20Fields%5D%20AND%20%28%22primates%22%5BMeSH%20Terms%5D%20OR%20Primates%5BText%20Word%5D%29%20NOT%20%22humans%22%5BMeSH%5D)]

Dynamic positron imaging of [^11^C]choline in a rhesus monkey showed a rapid brain uptake, followed by a rapid decline, with a heavy late uptake in muscle (10).

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Choline%5BAll%20Fields%5D%20AND%20human)]

A time-course study of a normal 60-year-old man with [^11^C]choline PET revealed the following organs with high [^11^C]choline uptake: kidney, liver, pancreas, small intestine content, and salivary gland. Dosimetry of [^11^C]choline in an ideal man was estimated (3). The total body absorbance dose was 0.00279 mSv/MBq (10.3 mrem/mCi). The kidneys (0.018 mGy/MBq (67 mrad/mCi)) received the highest dose of radioactivity, followed by the liver (0.017 mGy/MBq (63 mrad/mCi)), pancreas (0.013 mGy/MBq (48 mrad/mCi)), and spleen (0.008 mGy/MBq (30 mrad/mCi)). Various tumors of >1600 cancer patients were visualized with both [^11^C]choline and [^18^F]FDG (3). If the tumor was in an organ with high uptake, it was impossible to distinguish the tumor uptake from the normal organ uptake. If the tumor was separated from normal tissue uptake, [^11^C]choline PET visualized tumors as small as 5 mm in diameter, and FDG PET visualized tumors of 10 mm in diameter. Lung cancer and pulmonary tuberculosis could be differentiated by comparing [^11^C]choline PET and FDG PET images (11).

[^11^C]choline PET is a useful tool in diagnosis of brain tumor [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Choline%5BAll%20Fields%5D%20AND%20%22hominidae%22%5BMeSH%20Terms%5D%20AND%20%22brain%22%5BAll%20Fields%5D)], lung cancer [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Choline%5BAll%20Fields%5D%20AND%20%28%22human%22%5BMeSH%20Terms%5D%20OR%20%22hominidae%22%5BMeSH%20Terms%5D%20OR%20human%5BText%20Word%5D%29%20AND%20%28%22lung%22%5BMeS)], esophageal cancer (12), colorectal cancer (3), bladder cancer (13), and prostate cancer [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-Choline%5BAll%20Fields%5D%20AND%20%28%22human%22%5BMeSH%20Terms%5D%20OR%20%22hominidae%22%5BMeSH%20Terms%5D%20OR%20human%5BText%20Word%5D%29%20AND%20%22prostate%22%5BAll)].

## NIH Support

P50 CA128301, U54 CA119338, R01 CA122602-02

## References

1 DeGrado T.R., Baldwin S.W., Wang S., Orr M.D., Liao R.P., Friedman H.S., Reiman R., Price D.T., Coleman R.E. (2001). Synthesis and evaluation of (18)F-labeled choline analogs as oncologic PET tracers. J Nucl Med.
2 Podo F. (1999). Tumour phospholipid metabolism. NMR Biomed.
3 Hara T. (2002). 11C-choline and 2-deoxy-2-[18F]fluoro-D-glucose in tumor imaging with positron emission tomography. Mol Imaging Biol.
4 Tian M., Zhang H., Oriuchi N., Higuchi T., Endo K. (2004). Comparison of 11C-choline PET and FDG PET for the differential diagnosis of malignant tumors. Eur J Nucl Med Mol Imaging.
5 Rosen M.A., Jones R.M., Yano Y., Budinger T.F. (1985). Carbon-11 choline: synthesis, purification, and brain uptake inhibition by 2-dimethylaminoethanol. J Nucl Med.
6 Hara T., Kosaka N., Shinoura N., Kondo T. (1997). PET imaging of brain tumor with [methyl-11C]choline. J Nucl Med.
7 Hara T., Yuasa M. (1999). Automated synthesis of [11C]choline, a positron-emitting tracer for tumor imaging. Appl Radiat Isot.
8 Narayanan T.K., Said S., Mukherjee J., Christian B., Satter M., Dunigan K., Shi B., Jacobs M., Bernstein T., Padma M., Mantil J. (2002). A comparative study on the uptake and incorporation of radiolabeled methionine, choline and fluorodeoxyglucose in human astrocytoma. Mol Imaging Biol.
9 Zheng Q.H., Stone K.L., Mock B.H., Miller K.D., Fei X., Liu X., Wang J.Q., Glick-Wilson B.E., Sledge G.W., Hutchins G.D. (2002). [11C]Choline as a potential PET marker for imaging of breast cancer athymic mice. Nucl Med Biol.
10 Friedland R.P., Mathis C.A., Budinger T.F., Moyer B.R., Rosen M. (1983). Labeled choline and phosphorylcholine: body distribution and brain autoradiography: concise communication. J Nucl Med.
11 Hara T., Kosaka N., Suzuki T., Kudo K., Niino H. (2003). Uptake rates of 18F-fluorodeoxyglucose and 11C-choline in lung cancer and pulmonary tuberculosis: a positron emission tomography study. Chest.
12 Kobori O., Kirihara Y., Kosaka N., Hara T. (1999). Positron emission tomography of esophageal carcinoma using (11)C-choline and (18)F-fluorodeoxyglucose: a novel method of preoperative lymph node staging. Cancer.
13 de Jong I.J., Pruim J., Elsinga P.H., Jongen M.M., Mensink H.J., Vaalburg W. (2002). Visualisation of bladder cancer using (11)C-choline PET: first clinical experience. Eur J Nucl Med Mol Imaging.